# ^111^In-Diethylenetriamine pentaacetic acid-anti-epithelial glycoprotein-1 hRS7 humanized monoclonal antibody

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-anti-epithelial glycoprotein-1 hRS7 humanized monoclonal antibody
Abbreviated name: | ^111^In-DTPA-hRS7
Synonym:
Agent category: | Antibody
Target: | Epithelial glycoprotein-1 (EGP-1, also known as TROP2)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/ contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/ACR78188.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_002353.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4070) for more information about EGP-1

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7)]

Epithelial glycoprotein-1 (EGP-1, also known as TROP2) is a transmembrane glycoprotein (46 kDa) identified with murine IgG_1_ monoclonal antibody (mAb) RS7 raised against human non-small cell lung carcinoma (1). EGP-1 is also present in human carcinomas of the stomach, bladder, breast, ovary, uterus, and prostate, but it is not expressed in most normal tissues. EGP-1 is expressed at low levels in glandular cells in the bronchus, breast, prostate, skin, and pancreas. EGP-1 activates intracellular calcium mobilization (2) and protein kinase C (3) after binding with RS7. EGP-1 is a cell-surface receptor with unknown physiological ligand and cellular functions. However, EGP-1 has been implicated in the activation of the ERK/MAPK pathway, leading to downstream alterations in cellular proliferation, migration, invasion, and survival of cancer cells (4). EGP-1 overexpression has been associated with increased tumor invasiveness and decreased overall survival rates in multiple types of human carcinomas (5, 6). van Rij et al. (7) evaluated ^111^In-diethylenetriamine pentaacetic acid-hRS7 (^111^In-DTPA-hRS7) as a ^111^In-based single-photon emission computed tomography (SPECT) agent in human prostate PC-3 tumors in nude mice.

### Related Resource Links:

- Chapters in MICAD (EGP-1 (http://www.ncbi.nlm.nih.gov/books?term=(EGP-1%20OR%20EpCAM)%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGP-1 (http://www.ncbi.nlm.nih.gov/gene/4070))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGP-1 (http://www.ncbi.nlm.nih.gov/omim/137290))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+synthesis)]

DTPA-hRS7 was prepared by conjugation of p-isothiocyanatobenzyl-DTPA to hRS7 at a molar ratio of 50:1 (pH 9.5) for 60 min at 25°C (7). DTPA-hRS7 was purified with dialysis. There were two DTPA moieties per mAb. DTPA-hRS7 was incubated with ^111^InCl_3_ in 0.25 M NH_4_Ac buffer (pH 5.4) for 60 min at 25°C. ^111^In-DTPA-hRS7 was purified with column chromatography. The specific activity was estimated to be 606 MBq/nmol (16.4 mCi/nmol). No radiochemical yield or radiochemical purity was reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+in+vitro)]

Immunostaining of PC-3 tumor sections with hRS7 showed the expression of EGP-1 in the membranes and cytosol of PC-3 tumor cells (7). Immunochemical analysis of three human primary prostate tumor sections showed high homogeneous and consistent expression of EGP-1 in all three tumors and metastases in a lymph node and in the liver. The immunoreactivity of ^111^In-DTPA-hRS7 was >80%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+in+vitro)]

van Rij et al. (7) injected 0.4 MBq (0.011 mCi, 0.66 pmol) ^111^In-DTPA-hRS7 into male nude mice (n = 5/group) bearing the EGP-1–positive PC-3 human prostate tumors for ex vivo biodistribution studies. Ex vivo tumor accumulation was 61 ± 15% injected dose/gram (ID/g) at 3 d after injection. The tumor/blood ratio was 7.2. The radioactivity levels in the other organs were <10% ID/g. Co-injection of excess hRS7 (0.66 nmol) inhibited the accumulation in the tumors to 22 ± 7% ID/g and the tumor/blood ratio to 3.0 at 3 d after injection. Little inhibition was observed in the other organs.

van Rij et al. (7) performed ex vivo biodistribution and SPECT imaging studies in male nude mice (n = 5/group) bearing orthotopic PC-3 xenografts (17 d after tumor inoculation) at 3 d after injection of 37 MBq (1 mCi, 0.066 nmol)) ^111^In-DTPA-hRS7. Prostate tumor accumulation was 32 ± 13% ID/g. The radioactivity levels in the other organs were <7% ID/g, with <4% ID/g in the normal prostate. Co-injection of excess hRS7 (3.3 nmol) inhibited accumulation in the tumors to 6.1 ± 1.7% ID/g. Little inhibition was observed in the other organs. SPECT imaging showed that the tumors were clearly visualized in the prostate of all mice. The tumor/liver ratio was 7.3.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hRS7+AND+human)]

No publication is currently available.

## References

1 Stein R., Chen S., Sharkey R.M., Goldenberg D.M. (1990). Murine monoclonal antibodies raised against human non-small cell carcinoma of the lung: specificity and tumor targeting. Cancer Res.
2 Ripani E., Sacchetti A., Corda D., Alberti S. (1998). Human Trop-2 is a tumor-associated calcium signal transducer. Int J Cancer.
3 Basu A., Goldenberg D.M., Stein R. (1995). The epithelial/carcinoma antigen EGP-1, recognized by monoclonal antibody RS7-3G11, is phosphorylated on serine 303. Int J Cancer.
4 Cubas R., Zhang S., Li M., Chen C., Yao Q. (2010). Trop2 expression contributes to tumor pathogenesis by activating the ERK MAPK pathway. Mol Cancer.
5 Varughese J., Cocco E., Bellone S., de Leon M., Bellone M., Todeschini P., Schwartz P.E., Rutherford T.J., Pecorelli S., Santin A.D. (2011). Uterine serous papillary carcinomas overexpress human trophoblast-cell-surface marker (Trop-2) and are highly sensitive to immunotherapy with hRS7, a humanized anti-Trop-2 monoclonal antibody. Cancer.
6 Bignotti E., Todeschini P., Calza S., Falchetti M., Ravanini M., Tassi R.A., Ravaggi A., Bandiera E., Romani C., Zanotti L., Tognon G., Odicino F.E., Facchetti F., Pecorelli S., Santin A.D. (2010). Trop-2 overexpression as an independent marker for poor overall survival in ovarian carcinoma patients. Eur J Cancer.
7 van Rij C.M., Sharkey R.M., Goldenberg D.M., Frielink C., Molkenboer J.D., Franssen G.M., van Weerden W.M., Oyen W.J., Boerman O.C. (2011). Imaging of prostate cancer with immuno-PET and immuno-SPECT using a radiolabeled anti-EGP-1 monoclonal antibody. J Nucl Med.